# 5-(2-[^18^F]Fluoroethoxy)-L-tryphan

Chemical name: | 5-(2-[^18^F]Fluoroethoxy)-L-tryphan
Abbreviated name: | [^18^F]-L-FEHTP, 5-^18^FEHTP
Synonym: | L-5-(2-[^18^F]Fluoroethoxy)tryphan
Agent category: | Compound
Target: | L-type amino acid transporter 1 (LAT1)
Target category: | Amino acid uptake
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissues (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, S-[^11^C]methyl-L-methionine ([^11^C]MET), and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in oncological imaging (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter (LAT) system, a Na-dependent transporter system A, or a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their metabolic activities, including incorporation into proteins, which are higher than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6) but are not approved by the United States Food and Drug Administration. These agents are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell, except for leucine which is incorporated into proteins, quantitatively. These natural amino acid images are based on amino acid transport and protein incorporation.

5-(2-[^18^F]Fluoroethoxy)-L-tryphan ([^18^F]-L-FEHTP), unlike L-3,4-dihydroxy-6-[^18^F]fluorophenylalanine ([^18^F]FDOPA (http://www.ncbi.nlm.nih.gov/books/NBK23043/)), is only a substrate of LAT1 and is not a substrate of aromatic L-amino acid decarboxylase (AADC). [^18^F]-L-FEHTP was evaluated as a PET tumor imaging agent in mice with comparison to [^18^F]fluoro-2-deoxy-2-D-glucose ([18F]FDG (http://www.ncbi.nlm.nih.gov/books/NBK23335/)) and [^18^F]FDOPA (8, 9).

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter 1 (http://www.ncbi.nlm.nih.gov/gene/8140), L-type amino acid transporter 2 (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), L-[^11^C]methionine (http://google2.fda.gov/search?q=11C-methionine+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20and%20synthesis)]

[^18^F]-L-FEHTP was synthesized by direct alkylation of 5-hydroxy-L-tryptophan with [^18^F]fluoroethyltosylate for 10 min at 90°C (9). [^18^F]Fluoroethyltosylate was prepared by [^18^F]-fluorination of ethylene glycol-1,2-ditosylate with [^18^F]-potassium Kryptofix complex for 15 min at 100°C. This two-step automated synthesis provided [^18^F]-L-FEHTP with 12%–16% overall yield and a radiochemical purity >98% with a total synthesis time of ~40 min. The specific activities of [^18^F]-L-FEHTP was 50–150 GBq/μmol (1.35–4.05 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20and%20in%20vitro)]

Kramer et al. (8) showed that [^18^F]-L-FEHTP accumulation in NCI-H69 endocrine small cell lung cancer cells, PC-3 prostate cancer cells, and MDA-MB-231 breast cancer cells was reduced by >95% in the presence of 10 mM 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (BCH, an L-type transporter inhibitor). The radioactivity accumulation of [^18^F]-L-FEHTP was 48%–113% incubation dose (ID)/mg protein in the absence of BCH. The ADCC inhibitor S-carbidopa had little effect on the [^18^F]-L-FEHTP accumulation in these cells, suggesting that decarboxylation was not involved in the accumulation. On the other hand, S-carbidopa almost completely abolished the accumulation of [^18^F]FDOPA (26%–53% ID/mg protein).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20and%20rodentia)]

Ex vivo tissue accumulation of [^18^F]-L-FEHTP was studied in mice (n = 6/group) bearing S180 fibrosarcoma at 15, 30, 60, and 120 min after injection of 0.74 MBq (0.02 mCi) of the tracer as reported by Li et al. (9). The tumor accumulation of radioactivity was 3.07 ± 1.04% injected dose (ID)/g, 4.61 ± 1.18% ID/g, 5.19 ± 0.79% ID/g, and 2.37 ± 0.23% ID/g at 15, 30, 60, and 120 min, respectively. The tissue with the highest uptake was the liver (4.59%), followed by the kidney (4.05% ID/g), lung (3.86% ID/g), small intestine (3.65% ID/g), brain (3.18% ID/g), spleen (3.15% ID/g), heart (2.41% ID/g), muscle (2.04% ID/g), bone (1.94% ID/g), and blood (1.91% ID/g) at 30 min. All tissues showed moderate washout. The maximal tumor/blood and tumor/muscle ratios at 60 min were 2.87 and 2.79, respectively. [^18^F]-L-FEHTP remained >95% intact and no other radioactive metabolites were detected in the blood, brain, and tumors at 15 and 60 min after injection. No blocking studies were performed.

In a separate study, accumulation of [^18^F]-L-FEHTP (n = 4) and [^18^F]FDG (n = 4) was compared in mice with tumors and Staphylococcus aureus-induced inflammation in thigh muscle. [^18^F]-L-FEHTP exhibited tumor/muscle and inflammation/muscle ratios of 2.79 and 0.94, respectively, at 60 min after injection. On the other hand, [^18^F]FDG exhibited tumor/muscle and inflammation/muscle ratios of 2.91 and 3.17, respectively, at 60 min after injection. Whole-body PET imaging at 60 min after injection showed high [^18^F]-L-FEHTP and [^18^F]FDG accumulation in the tumors, whereas low [^18^F]-L-FEHTP and high [^18^F]FDG accumulation were observed in the inflammation.

Kramer et al. (8) performed ex vivo biodistribution studies in nude mice bearing NCI-H69 (n = 3) or PC-3 xenografts (n = 4) at 70 min after injection of [^18^F]-L-FEHTP. The tumor accumulation of radioactivity (standard uptake value (SUV)) was 1.58 ± 0.48 and 1.40 ± 0.35 in the NCI-H69 and PC-3 tumors, respectively. The tissue with the highest SUV was the pancreas (8.50), followed by the kidney (2.05), spleen (0.88), brain (0.84), liver (0.81), heart (0.78), and blood (0.75). Pretreatment with tryptophan (25 mg/kg, 10 min) resulted in a slight decrease (not significant) of tissue accumulation in the NCI-H69 tumors, brain, and kidneys but had little effect on the other tissues.

Kramer et al. (8) performed PET imaging studies in mice (n = 3–7/group) bearing NCI-H69 or PC-3 tumors after injection of [^18^F]-L-FEHTP or [^18^F]FDOPA. Dynamic and static PET scans showed the accumulation of both tracers in the two tumors with SUV of ~1.5. Pretreatment with S-carbidopa 60 min before [^18^F]FDOPA decreased the radioactivity levels in the PC-3 tumors by ~50%, whereas no decrease was observed in the accumulation of [^18^F]-L-FEHTP.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEHTP%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Kramer S.D., Mu L., Muller A., Keller C., Kuznetsova O.F., Schweinsberg C., Franck D., Muller C., Ross T.L., Schibli R., Ametamey S.M. (2012). 5-(2-18F-fluoroethoxy)-L-tryptophan as a substrate of system L transport for tumor imaging by PET. J Nucl Med.
9 Li R., Wu S.C., Wang S.C., Fu Z., Dang Y., Huo L. (2010). Synthesis and evaluation of l-5-(2-[(18)F]fluoroethoxy)tryptophan as a new PET tracer. Appl Radiat Isot.